# 6-Fluoropyridoxol

Chemical name: | 6-Fluoropyridoxol
Abbreviated name: | 6-FPOL
Synonym: | 2-Fluoro-5-hydroxy-6-methyl-3,4-pyridinedimethanol, 2-fluoro-3,4-di(hydroxymethyl)-5-hydroxy-6-methyl-pyridine
Agent Category: | Compound
Target: | Proton (H^+^)
Target Category: | Protonation and deprotonation of the 3-phenolic OH in different pH environments that lead to chemical shift changes of ^19^F at the 6 position.
Method of detection: | ^19^F-Magnetic Resonance Spectroscopy (MRS)
Source of signal/contrast: | ^19^F
Activation: | No
Studies: | - In vitro; - Rodents | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=6-fluoropyridoxol%20OR%206-FPOL)]

6-Fluoropyridoxol (6-FPOL) is a fluorinated vitamin B_6_ derivative developed for measuring transmembrane pH gradient in vivo with ^19^F magnetic resonance spectroscopy (^19^F-MRS) (1, 2).

Magnetic resonance imaging and MRS imaging are evolving nuclear magnetic resonance (NMR) techniques that can be used for non-invasive evaluation of anatomic and metabolic features of pathologies (3, 4). MRS can detect metabolites that contain proton, phosphorus, fluorine, or other nuclei. Both ^1^H- and ^31^P-MRS have revealed significant disturbances in amino acids, lipids, and phosphorus-containing metabolites in vivo (5, 6). Cellular pH has been found to play a regulatory role in most cellular processes, from the activity of individual enzymes to coordinated development of an organism (7). Many metabolic enzymes exhibit optimal activity in a narrow pH range. There are also significant pH gradients within and between cellular compartments. Compared with normal tissue, tumor tissue has a reversed pH gradient with an acidic extracellular compartment and a basic intracellular compartment. Mechanical activity of the heart is greatly influenced by pH, and myocardial ischemia can lead to hypoxia and acidosis. Clinically, MRS can be used to monitor cellular pH and detect pH changes in response to therapy. Theoretically, MRS chemical shift imaging may allow in vivo mapping of tissue/organ pH changes.

Many molecules exhibit chemical shift response to pH changes, and measurements of these chemical shifts are directly related to pH (7). In vivo MRS pH measurement can be performed with endogenous molecules such as inorganic phosphate in ^31^P-MRS. However, pH measurement in whole tissues by use of endogenous molecules is not always successful because of crowded spectra, broad lines, or low molecule concentrations. Exogenous molecules have been found to be useful as reporter probes to facilitate in vivo pH measurement. Among these molecules, ^19^F-MRS chemical shift molecules have distinct advantages of a large chemical shift range, high gyromagnetic ratio, high detection sensitivity, and no background signal from tissues. Mason (7) studied various fluorinated vitamin B_6_ analogs as ^19^F-MRS agents to measure intracellular pH (pH_i_) and extracellular pH (pH_e_). Mehta et al. (2) evaluated one of these analogs, 6-FPOL, and found that the molecule exhibited exceptional sensitivity to changes in pH and could be used to measure pH_i_ and pH_e_ simultaneously. The response of ^19^F-MRS chemical shifts to pH in the molecule is considered to be caused primarily by protonation and deprotonation of the 3-phenolic OH. This affects the electronic environment around fluorine at position 6, which is very pronounced because of the para location.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%286-fluoropyridoxol%20OR%206-FPOL%29%20AND%20synthesis)]

Korytnyk and Srivastava (8) first reported the synthesis of 6-halogen-substituted vitamin B_6_ analogs. Mason (7) described it in three steps starting from pyridoxine hydrochloride. Diazotization of pyridoxine with benzene diazonium chloride gave 6-phenazopyridoxol. Dithionite reduction or catalytic reduction (Pd/C) produced 6-aminopyridoxol. 6-FPOL was then produced from 6-aminopyridoxol by a modified Schieman reaction. Specifically, 6-aminopyridoxol in 40% HBF_4_ was reacted with NaNO_2_ at 10 °C for 2 h. After addition of 5 N NaOH at 10 °C to pH 3-4, the solution was extracted with diethyl ether, washed with water, dried, and concentrated. The crystalline material was recrystallized from diethyl ether. The final yield was 34%.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%286-fluoropyridoxol%20OR%206-FPOL%29%20AND%20in%20vitro)]

Mehta et al. (2) used 7-Tesla (282.3 MHz) NMR to study 6-FPOL in fresh whole blood obtained from rabbits. 6-FPOL exhibited a single sharp ^19^F-NMR resonance in aqueous solution or plasma with a line width of ~20 Hz. The ^19^F-NMR chemical shift of 6-FPOL was very sensitive to pH with a change of 9.76 ppm between acid and base. Coefficients of the Henderson-Hasselbach equation were determined as pKa = 8.2, δ (acid) = –9.85 ppm, and δ (base) = –19.61 ppm. 6-FPOL produced two distinct, well-resolved ^19^F-NMR resonances at –10.72 ± 0.03 ppm (intracellular compartment) and –11.34 ± 0.06 ppm (extracellular compartment), which corresponded to pH 7.19 ± 0.02 and 7.45 ± 0.02, respectively. The molecule had a chemical shift range of ~10 ppm. The pH-dependent ^19^F-NMR chemical shift of 6-FPOL was independent of temperature and the presence of metal ions or plasma proteins. 6-FPOL penetrated and left the red blood cells rapidly, but exchange was sufficiently slow to provide separate resonances for intra- and extracellular compartments. Acid-base exchange was in the fast-exchange regime so that a single narrow line was observed for each compartment. In a separate experiment using blood saturated with carbon monoxide to reduce intracellular paramagnetic line broadening from deoxyhemoglobin, ^31^P-NMR indicated an intracellular pH ~7.14 ± 0.06.

Hunjan et al. (9) evaluated 6-FPOL in perfused rat hearts, using a 9.4-Tesla NMR (376 MHz) spectrometer. The addition of 6-FPOL to a single heart showed two well-resolved peaks at –10.63 ± 0.01 ppm (intracellular compartment; n = 3 repeated measurements) and –11.53 ± 0.04 ppm (extracellular compartment), corresponding to pH_i_ = 7.14 ± 0.01 and pH_e_ = 7.52 ± 0.02, respectively. In eight hearts, the measurements were similar, in the range of –10.43 to –10.69 ppm (intracellular compartment) and –11.50 to –12.45 ppm (extracellular compartment), corresponding to mean pH_i_ of 7.11 ± 0.07 and pH_e_ of 7.60 ± 0.08, respectively. The ^31^P-NMR chemical shift of inorganic phosphate gave similar measurements for pH_i_ (7.11 ± 0.04; n = 7), and external electrode measurement gave a pH_e_ of 7.63 ± 0.33 (n = 5). On addition of 6-PFOL (3.6 mM), hearts occasionally showed an immediate but transient 10-40% reduction in developed pressure, lasting 3-6 min, followed by complete recovery. 6-FPOL ^19^F-MRS showed the changes in pH_i_ and pH_e_ when artificial metabolic alkalosis or acidosis was induced by sodium hydroxide or hydrochloric acid. In both instances, pH_e_ changed significantly but pH_i_ remained unchanged. In respiratory alkalosis induced by reducing the CO_2_ concentration from 5% to 0%, both pH_i_ and pH_e_ changed simultaneously. Total global ischemia induced by halting the flow of perfusate caused the intracellular and extracellular peaks to merge together as an indication of acidosis.

He et al. (1) studied 6-FPOl and a series of fluorinated vitamin B_6_ analogs in whole blood and perfused rat hearts, using a 7-Tesla (282 MHz) NMR spectrometer. They found that the pyridine core of vitamin B_6_ was readily amenable to many chemical modifications. The modification of the 4- and 5- position hydroxymethyl moieties produced modification of the pKa with relatively minor changes in chemical shift and chemical shift range. The introduction of an aminomethyl group at these positions appeared to cause the pKa to shift toward the acidic range. The introduction of the electron-withdrawing carboxyl group caused a shift toward base.

Korytnyk and Srivastava (8) found that 6-FPOL appeared to inhibit in vitro growth of tumor cells with an inhibitory concentration (ID_50_) of ~0.1 mM for adenocarcinoma (TA-3) cells and 25 μM for sarcoma (S-180) cells.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%286-fluoropyridoxol%20OR%206-FPOL%29%20AND%20rodentia)]

Korytnyk and Srivastava (8) injected a single i.p. dose of 6-FPOL in mice and found that the mice survived a dose of 100 mg/kg

Mason (7) reported that transmembrane pH gradient of tumors could be measured by ^19^F-MRS in rats bearing Dunning AT1 prostate rat tumors after i.p administration of 6-FPOL (200 mg/rat; ~800 mg/kg) with no obvious acute toxicity.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22%20SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28primate%20NOT%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20human)]

No publication is currently available.

## NIH Support

NIH Biotechnology Facility Grant #5-P41-RR02584, CA-08793, CA-13038, R01CA79515.

## References

1 He S., Mason R.P., Hunjan S., Mehta V.D., Arora V., Katipally R., Kulkarni P.V., Antich P.P. (1998). Development of novel 19F NMR pH indicators: synthesis and evaluation of a series of fluorinated vitamin B6 analogues. Bioorg Med Chem.
2 Mehta V.D., Kulkarni P.V., Mason R.P., Constantinescu A., Aravind S., Goomer N., Antich P.P. (1994). 6-Fluoropyridoxol: a novel probe of cellular pH using 19F NMR spectroscopy. FEBS Lett.
3 Kuroda K. (2005). Non-invasive MR thermography using the water proton chemical shift. Int J Hyperthermia.
4 Golder W. (2004). Magnetic resonance spectroscopy in clinical oncology. Onkologie.
5 Bolan P.J., Nelson M.T., Yee D., Garwood M. (2005). Imaging in breast cancer: Magnetic resonance spectroscopy. Breast Cancer Res.
6 Imamura K. (2003). Proton MR spectroscopy of the brain with a focus on chemical issues. Magn Reson Med Sci.
7 Mason R.P. (1999). Transmembrane pH gradients in vivo: measurements using fluorinated vitamin B6 derivatives. Curr Med Chem.
8 Korytnyk W., Srivastava S.C. (1973). Synthesis and physicochemical and biological properties of 6-halogen-substituted vitamin B 6 analogs. J Med Chem.
9 Hunjan S., Mason R.P., Mehta V.D., Kulkarni P.V., Aravind S., Arora V., Antich P.P. (1998). Simultaneous intracellular and extracellular pH measurement in the heart by 19F NMR of 6-fluoropyridoxol. Magn Reson Med.